# ^99m^Tc-1,4,7-Tris(carboxymethyl)-10-(4-aminoethyl)-1,4,7,10-tetraazacyclododecane-Folate

Chemical name: | ^99m^Tc-1,4,7-Tris(carboxymethyl)-10-(4-aminoethyl)-1,4,7,10-tetraazacyclododecane-Folate
Abbreviated name: | ^99m^Tc-DO3A-EA-Folate
Synonym:
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate)]

Folic acid is a water-soluble B vitamin (1). It is essential for methylation and DNA synthesis. The primary pathway for entry of folate into cells is through a facilitated transporter, which has a low affinity for folate (K_m_, 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a receptor with higher affinity (K_d_, 0.5 nM), which allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate receptors (2). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpressed the high-affinity folate receptor but to a lesser frequency (20%–50%). Several ^99m^Tc-based folate conjugates have been developed for single-photon emission computed tomography (SPECT) imaging of folate receptor expression in tumors such as ^99m^Tc-ethylenedicysteine-folate (http://www.ncbi.nlm.nih.gov/books/NBK23152/), ^99m^Tc-HYNIC-Folate, and ^99m^Tc-DTPA-Folate (3). Mishra et al. (4) prepared ^99m^Tc-1,4,7-tris(carboxymethyl)-10-(4-aminoethyl)-1,4,7,10-tetraazacyclododecane-folate (^99m^Tc-DO3A-EA-Folate) as a new ^99m^Tc-based folate conjugate for SPECT imaging studies.

### Related Resource Links:

- Chapters in MICAD (folate receptor (http://www.ncbi.nlm.nih.gov/books?term=folate%20receptor%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (folate receptor (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor))
- Drug information in FDA (folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20AND%20synthesis%5BAll%20Fields%5D%29)]

^99m^Tc was complexed efficiently (>97% yield) to DO3A-EA-folate to form ^99m^Tc-DO3A-EA-folate, with a radiochemical purity of >97% (4). The specific activity was calculated to be ~2 μCi/μg (0.074 MBq/μg) before in vivo injection in mice. ^99m^Tc-DO3A-EA-Folate was found to be stable in human serum for up to 24 h at 37ºC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20AND%20folate%20and%20in%20vitro)]

Receptor binding studies were performed using human oral carcinoma KB, ovarian carcinoma OAW, and malignant glioma U87MG cells with ^99m^Tc-DO3A-EA-folate (4). The affinity binding constant (K_d_) values were calculated to be 4.2 ± 0.8, 22.5 ± 0.1, and 16.7 ± 0.1 µM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20and%20rodentia)]

Nude mice (number of mice studied not reported) were inoculated with KB tumor cells, followed by intravenous injection of 3.7 MBq (0.1 mCi) ^99m^Tc-DO3A-EA-folate 14–17 days after tumor transplantation (4). Ex vivo biodistribution studies were performed at 1, 4, and 24 h after injection. Tumor accumulation was 5.06% injected dose/g (ID/g) at 1 h, 6.26 ± 0.40% ID/g at 4 h, and 4.06 ± 0.32% ID/g at 24 h. The organ with the highest accumulation was the liver (17.6% ID/g), followed by the kidney (15.0% ID/g), intestines (4% ID/g), and spleen (4% ID/g) at 1 h after injection, with <1% at 24 h. The blood, heart, lung, stomach, and muscle showed <2% ID/g at 1–24 h. The tumor/blood ratios were 2.3 ± 0.3 and 6.1 ± 1.0 at 1 h and 4 h after injection, respectively. There was a biphasic clearance of ^99m^Tc-DO3A-EA-folate in the blood, with half-life values of 12 min and 140 min. Co-injection with unlabeled folate blocked the uptake of ^99m^Tc-DO3A-EA-folate by 67%, 50%, and 60% in the tumor, kidney, and liver, respectively, at 4 h after injection.

Scintigraphic images of mice injected with 3 MBq (0.08 mCi) ^99m^Tc-DO3A-EA-folate showed that tumors in the right hind legs could be well visualized at 1–4 h (4). The tumor/muscle ratios were estimated to be 11.8 ± 1.2 and 19.7 ± 3.3 at 1 h and 4 h, respectively. ^99m^Tc-DO3A-EA-folate could be a useful tool for imaging tumors positive for folate receptor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20folate%20and%20%28primates%20not%20humans%29)]

No publication is currently available

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=99mTc-DO3A-EA-folate%20and%20humans)]

No publication is currently available.

## References

1 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
2 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
3 Ilgan S., Yang D.J., Higuchi T., Zareneyrizi F., Bayhan H., Yu D., Kim E.E., Podoloff D.A. (1998). 99mTc-ethylenedicysteine-folate: a new tumor imaging agent. Synthesis, labeling and evaluation in animals. Cancer Biother Radiopharm.
4 Mishra G., Hazari P.P., Kumar N., Mishra A.K. (2011). In vitro and in vivo evaluation of (99m)Tc-DO3A-EA-Folate for receptor-mediated targeting of folate positive tumors. J Drug Target.